# ^64^Cu-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-VENK[homoC]NKEMRNRYWEAALDPNLNNQQKRAKIRSIYDDP[homoC]-NH_2_ with a disulfide bridge between the two homoC

Chemical name: | ^64^Cu-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-VENK[homoC]NKEMRNRYWEAALDPNLNNQQKRAKIRSIYDDP[homoC]-NH_2_ with a disulfide bridge between the two homoC | [image]
Abbreviated name: | ^64^Cu-DOTA-MUT-DS | [image]
Synonym: | | [image]
Agent Category: | Affibody, antibody | [image]
Target: | HER2 | [image]
Target Category: | Receptor | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^64^Cu | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of ^64^Cu/^111^In-DOTA-MUT-DS by Ren et al. (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=affibody%20and%20HER2%20and%20molecular%20imaging)]

The ^64^Cu-labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA)-VENK[homoC]NKEMRNRYWEAALDPNLNNQQKRAKIRSIYDDP[homoC]-NH_2_ (MUT-DS) conjugate with a disulfide bridge between the two homocysteines, abbreviated as ^64^Cu-DOTA-MUT-DS, is a 2-helix affibody derivative that was synthesized by Ren et al. for positron emission tomography (PET) of HER2-expressing tumors (1).

Affibody molecules are a group of nonimmunogenic scaffold proteins that are derived from the B-domain of staphylococcal surface protein A (2, 3). These molecules have only 58 amino acid residues (~7 kDa), which form a 3-α-helical bundle structure (3, 4). Helices 1 and 2 bundles are responsible for the high binding affinity and specificity of affibodies to their targets, while helix 3 contributes to the affibody stabilization and is not involved in receptor recognition (4). Studies have further confirmed that the binding domain in the helices 1 and 2 bundles includes 13 amino acid residues that are surface-exposed (2). Therefore, large affibody libraries have been constructed by randomization of the 13 amino acid residues, and a large set of affibody molecules against a wide variety of targets have been selected from those libraries. Of them, the affibodies specific to HER2, including Z_HER2:342_ and Z_HER2:477_, have been intensively investigated in recent years (3, 5). These molecules have been radiolabeled and tested for molecular imaging of HER2-expressing tumors.

The investigators at Stanford University first tested the feasibility of the monomeric (~7 kDa) and dimeric (~14 kDa) forms of affibody Z_HER2:477_ for molecular imaging (6, 7). Both forms have been labeled with various radioisotopes through chelating agents. Studies have shown that smaller affibody constructs perform better in vivo in terms of tumor uptake and clearance, which prompts them to generate smaller proteins with only α-helices 1 and 2 bundles (~4 kDa) (4, 6, 7). However, simple deletion of the helix 3 leads to significantly decreased binding affinity of the proteins because of decreased helix conformation (4). The investigators then applied various strategies to improve the helix conformation of the affibody molecules, including sequence mutation, placement of disulfide bridges, and inclusion of helix-promoting amino acids (4). Although the helix conformation (~15%, the amount of α-helix represented in the secondary structure of the affibodies) of the 2-helix molecules is still much lower than that of the parent 3-helix affibodies, the investigators successfully obtained a class of 2-helix small proteins with HER2-binding affinity up to 5 nM with these strategies (1, 8, 9). One of these 2-helix proteins is MUT-DS, which has α-helices 1 and 2 bundles with a disulfide bridge being formed between the two inserted homocysteines (4). The radiolabeled MUT-DS derivatives exhibited favorable pharmacokinetics for imaging HER2-expressing tumors. ^68^Ga-DOTA-MUT-DS, ^64^Cu-DOTA-MUT-DS, ^111^In-DOTA-MUT-DS, and ^18^F-FBO-MUT-DS are examples of the MUT-DS derivatives (1, 8, 9).

This chapter summarizes the data obtained with ^64^Cu-DOTA-MUT-DS (1).

### Related Resource Links:

- Anti-HER2 affibody conjugates in MICAD:

^68^Ga-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/books/NBK48901/), ^111^In-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/books/NBK23176/), Alexa750-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK45127/), ^111^In-benzyl-DOTA-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK23058/), ^111^In-benzyl-DTPA-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK23322/), Eaff800 (http://www.ncbi.nlm.nih.gov/books/NBK45665/), DY-682-ABD-Z_HER2:342_ (Haff682) (http://www.ncbi.nlm.nih.gov/books/NBK45664/), ^99m^Tc-Z_2395_-C (http://www.ncbi.nlm.nih.gov/books/NBK23590/), [^111^In]-ABY-025 (http://www.ncbi.nlm.nih.gov/books/NBK45623/), ^111^In-BZ-DTPA-Z_EGFR:1907_ (http://www.ncbi.nlm.nih.gov/books/NBK23654/).

- HER2-related clinical trials for imaging and therapy (http://clinicaltrials.gov/ct2/results?term=HER2)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21984380)]

Ren et al. generated the cyclic 2-helix small protein DOTA-MUT-DS with standard solid-phase peptide synthesis and I_2_ oxidation of the two inserted homocysteines (1). The DOTA-MUT-DS product was purified with high-performance liquid chromatography (HPLC). The chemical yield of DOTA-MUT-DS was ~10% with >95% purity. The measured molecular weight was 5,136.77 (calculated 5,136.53).

DOTA-MUT-DS was radiolabeled with ^64^Cu by reaction with ^64^CuCl_2_ in NaOAc buffer for 40 min at 40°C (1). After purification, the radiolabeled ^64^Cu-DOTA-MUT-DS had a >95% radiochemical purity. The specific activity was 3.98–6.83 MBq/nmol (0.11–0.18 mCi/nmol) at the end of synthesis. The intact radiolabeled complex was maintained >95% after 1 h incubation with mouse serum at 37°C, indicating good in vitro stability.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21984380)]

The binding affinity with HER2 antigen and the HER2-targeting ability in cultured SKOV3 human ovarian cancer cells for DOTA-MUT-DS were measured in vitro, and the results have been presented in another report and are also summarized in the MICAD chapter of ^68^Ga-DOTA-MUT-DS (9). The binding affinity of ^64^Cu-DOTA-MUT-DS was not reported.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21984380)]

The biodistribution of ^64^Cu-DOTA-MUT-DS was examined in mice bearing SKOV3 tumors after tail vein injection of 0.69–1.01 MBq (18.7–27.4 μCi) of the probe (1). Mice were euthanized at 1, 4, and 20 h after injection (n = 3 mice/time point). The results showed that ^64^Cu-DOTA-MUT-DS rapidly accumulated in tumors at early time points (4.66 ± 0.38% injected dose per gram tissue (ID/g) at 1 h after injection). The radioactivity in tumors reduced slightly to 3.34 ± 0.89% ID/g at 4 h and then slowly washed out from the tumors (2.13 ± 1.11% ID/g at 20 h after injection). The blood level was 1.54 ± 0.18% ID/g at 1 h and remained at 1.1 ± 0.02% ID/g at 20 h after injection. The highest tumor/blood ratio (3.05 ± 0.3) was obtained at 1 h after injection. On the contrary, the tumor/muscle ratios increased from 3.48 ± 0.53 at 1 h to 5.56 ± 2.15 at 4 h and then decreased to 3.72 ± 1.65 at 20 h after injection. Significantly high renal uptake (254.2 ± 19.1% ID/g) was observed at 1 h, and the activity then washed out to 137.7 ± 17.3% at 4 h and 24.97 ± 8.03% ID/g at 20 h after injection. The liver uptake values were 27.76 ± 6.4, 13.39 ± 3.65, and 13.39 ± 3.65% ID/g at 1, 4, and 20 h after injection, respectively.

Blocking studies were performed in tumor-bearing mice (n = 3) with co-injection of ^64^Cu-DOTA-MUT-DS with 300 μg unlabeled Z_HER2:477_ (1). Mice were euthanized at 4 h after injection. Co-injection with unlabeled Z_HER2:477_ significantly reduced the tumor uptake of ^64^Cu-DOTA-MUT-DS to 1.76 ± 0.12% ID/g with 48.2% inhibition (P < 0.05). Co-injection also decreased the tumor/blood and tumor/muscle ratios to 1.36 ± 0.04 and 3.73 ± 1.65, respectively. Although renal and liver uptakes also decreased, the uptake levels were not significantly different compared with those of the unblocked group (n = 3 mice) (P > 0.05).

PET imaging of a tumor-bearing mouse was performed at different times (0.5, 1, 2, 4, and 20 h) after injection of ^64^Cu-DOTA-MUT-DS (1 MBq (27 μCi)) (1). Tumors were clearly visualized on images, with good tumor/background contrast from 0.5 h to 20 h after injection. Consistent with the findings of the biodistribution study, high radioactivity was observed in the kidney region. In the mice co-injected with 300 μg unlabeled Z_HER2:477_ and imaged at 4 h after co-injection (n = 3 mice), unlabeled Z_HER2:477_ significantly blocked the uptake of ^64^Cu-DOTA-MUT-DS in the tumors (by 48.2%), resulting in a much lower tumor/background contrast.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are available.

## References

1 Ren, G., J.M. Webster, Z. Liu, R. Zhang, Z. Miao, H. Liu, S.S. Gambhir, F.A. Syud, and Z. Cheng, In vivo targeting of HER2-positive tumor using 2-helix affibody molecules. Amino Acids, 2011
2 Friedman M., Nordberg E., Hoiden-Guthenberg I., Brismar H., Adams G.P., Nilsson F.Y., Carlsson J., Stahl S. (2007). Phage display selection of Affibody molecules with specific binding to the extracellular domain of the epidermal growth factor receptor. Protein Eng Des Sel.
3 Orlova A., Feldwisch J., Abrahmsen L., Tolmachev V. (2007). Update: affibody molecules for molecular imaging and therapy for cancer. Cancer Biother Radiopharm.
4 Webster J.M., Zhang R., Gambhir S.S., Cheng Z., Syud F.A. (2009). Engineered two-helix small proteins for molecular recognition. Chembiochem.
5 Gao J., Chen K., Miao Z., Ren G., Chen X., Gambhir S.S., Cheng Z. (2011). Affibody-based nanoprobes for HER2-expressing cell and tumor imaging. Biomaterials.
6 Cheng Z., De Jesus O.P., Kramer D.J., De A., Webster J.M., Gheysens O., Levi J., Namavari M., Wang S., Park J.M., Zhang R., Liu H., Lee B., Syud F.A., Gambhir S.S. (2010). 64Cu-labeled affibody molecules for imaging of HER2 expressing tumors. Mol Imaging Biol.
7 Cheng Z., De Jesus O.P., Namavari M., De A., Levi J., Webster J.M., Zhang R., Lee B., Syud F.A., Gambhir S.S. (2008). Small-animal PET imaging of human epidermal growth factor receptor type 2 expression with site-specific 18F-labeled protein scaffold molecules. J Nucl Med.
8 Miao Z., Ren G., Jiang L., Liu H., Webster J.M., Zhang R., Namavari M., Gambhir S.S., Syud F., Cheng Z. (2011). A novel (18)F-labeled two-helix scaffold protein for PET imaging of HER2-positive tumor. Eur J Nucl Med Mol Imaging.
9 Ren G., Zhang R., Liu Z., Webster J.M., Miao Z., Gambhir S.S., Syud F.A., Cheng Z. (2009). A 2-helix small protein labeled with 68Ga for PET imaging of HER2 expression. J Nucl Med.